# 2´-Deoxy-2´-[^18^F]fluoro-5-fluoro-1-β-D-arabinofuranosyluracil

Chemical name: | 2´-Deoxy-2´-[^18^F]fluoro-5-fluoro-1-β-D-arabinofuranosyluracil
Abbreviated name: | [^18^F]FFAU
Synonym:
Agent Category: | Compound
Target: | Herpes simplex virus thymidine kinase (HSV-tk)
Target Category: | Phosphorylation
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%5BAll%20Fields%5D%20AND%20FFAU%5BAll%20Fields%5D)]

Herpes simplex virus type-1 thymidine kinase (HSV1-tk) can be used as a suicide gene for gene therapy. As of today, animal studies using HSV1-tk gene and ganciclovir (1) have brought some success in treating malignant tumors with suicide gene therapy; however, clinical results showed that such methods did not provide sufficient gene delivery to the tumor human cells for therapy (2).

HSV1-tk can phosphorylate a wide range of nucleoside analogs (e.g. acycloguanosines and 2'-deoxyfuranosyluracil nucleoside derivatives) that are not phosphorylated efficiently by the native enzyme (3). The presence of fluorine in the 2'-arabino position in a furanosyluracil nucleoside results in enhanced monophosphorylation by HSV-tk type 1 and type 2 compared with the host thymidine kinase.

In vivo imaging methods are essential tools for monitoring the gene expression as an indicator of gene delivery and for quantifying the level of HSV1-tk enzyme activity after gene transfer (4-6). Several probes for positron emission tomography (PET) of HSV1 -tk gene have been studied so far. Among them, [^18^F]FMAU, [^18^F]FHPG (7), [^18^F]FHBG and [^18^F]FIAU. [^124^I]FIAU appears to be superior to the acycloguanosine derivatives FHPG and FHBG in some cell lines (8) with respect to total uptake and the uptake ratio (tk-positive to wild type), although it is susceptible to deiodination in vivo. 2'-deoxy-2'-fluoro-5-fluoro-1-α-D-arabinofuranosyluracil ([^18^F]FFAU) may offer an advantage over [^124^I]FIAU and other 5-substituted analogs for imaging gene expression, and is currently under investigation (9).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%29FFAU%20AND%20synthesis)]

Alauddin et al. (9) synthesized [^18^F]FFAU by reaction of the respective triflate (2-deoxy-2-trifluoromethanesulfonyl-1,3,5-tri-O-benzoyl-α-D-ribofuranose with tetrabutylammonium [^18^F]fluoride. This reaction produced 2-[^18^F]-fluoro-1,3,5-tri-O-benzoyl-α-D-arabinofuranose, which was converted to its 1-bromo derivative by treatment with hydrogen bromide in acetic acid (HBr/AcOH). After coupling with protected 5-fluorouracil, the resulting product was hydrolyzed (in base) and purified by high-performance liquid chromatography (HPLC) to obtain the desired product [^18^F]FFAU.

[^18^F]FFAU was produced with a radiochemical yield of 20%-30% (decay-corrected with an average of 25% in 4 runs), and a radiochemical purity >99%. The average specific activity for [^18^F]FFAU was 85 GBq/µmol (2,300 mCi/ µmol) at the end of the synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%29FFAU%20AND%20in%20vitro)]

In vitro studies performed by Alauddin et al. (9) showed that the total accumulation of [^3^H]FFAU in HSV1-tk-expressing cells was significantly higher than that in wild-type control cells, and increased rapidly in the transduced cells, reaching a plateau by 60 min. Maximum incorporation of FFAU within a short time (30 min) suggested that the rate of monophosphorylation by the HSV1-tk was also very high. This was further supported by dynamic PET scans, which showed that tumor uptake peaked within 10 min of injection and remained elevated throughout the time course studied (see Rodents section).

The in vitro uptake ratios obtained between transduced and wild-type control cells were 176, 126, and 81 at 30, 60, and 120 min respectively. Tumor of [^3^H]FFAU in tk-positive cells was approximately 180-fold (P < 0.001) higher than those obtained in previous studies using 2'-[^14^C]-deoxy-2'-fluoro-5-methyl-1-β-D-arabinofuranosyluracil ([^14^C]FMAU) and 9-(4-[^18^F]-fluoro-3-hydroxymethylbutyl)guanine ([^18^F]FHBG) in the same cell lines (7).

In their studies, Allaudin et al. (9) reported a gradual and slow accumulation of FFAU in wild-type cells likely representing minimal baseline monophosphorylation by host kinase and irreversible binding to thymidylate synthase (TS) (10) throughout the 2 h study period. However, no significant increase in uptake in transduced cells was observed after 60 min, and the ratio between tk-positive and wild-type cells decreased from 176 to 81 by 2 h.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%29FFAU%20AND%20rodentia%5BMeSH%5D)]

Allaudin et al. (9) performed ex vivo studies of [^3^H]FFAU and in vivo PET studies of [^18^F]FFAU on 6- week-old athymic tumor-bearing nude mice (Harlan). For the ex vivo studies, one group of mice (n = 6) was injected intravenously via a tail vein with [^3^H]FFAU (37 kBq, 1 µCi, 200 µl), and blood samples were collected for 3 of them at 2, 5, 10, 20, 60, and 120 min post injection. The activity for each sample was calculated as a percentage of the injected dose per gram (% ID/g). At 2 h after injection, mice were sacrificed, and the activity was measured on excised tumors and organs using the external standard method of quench correction.

For in vivo PET studies of [^18^F]FFAU, mice (n = 2) were injected with 7.4 MBq (0.2 mCi) of [^18^F]FFAU, through the tail vein, and imaging was performed at 30 min, 1 h, and 2 h after injection. The radioactivity uptake in tumor (kBq/cm^3^, µCi/cm^3^) was converted to % ID/g and compared with the biodistribution data using [^3^H]FFAU. The higher uptake obtained in transduced tumor suggested an accumulation of [^18^F]FFAU, probably resulting from reversible binding to - or complex formation with- HSV-tk with net intracellular substrate trapping. Contrary to [^18^F]FMAU, no significant uptake in wild-type tumors was observed, suggesting that [^18^F]FFAU underwent only minimal phosphorylation by the host kinase during the 2 h time period.Results showed that tumor uptake in transduced cells was much higher than that in nontransduced cells. The values obtained for [^3^H]FFAU in transduced and wild-type tumors were 30.75 ± 7.43%ID/g and 3.87 ± 1.80% ID/g, respectively. The uptake in other organs, including blood, was quite low, except kidney, which appeared slightly higher with renal clearance as the primary route of radiotracer excretion.

Comparative studies between FFAU, FMAU, and FHBG on the cell line HT-29 showed that the total uptake of [^3^H]FFAU in vivo (% ID/g) was much higher compared with that of FMAU and FHBG, and that the uptake ratio between transduced and wild-type cells at 2 h for FFAU was also higher than that of FMAU and FHBG. On the other hand, the ratio was comparable between FHBG and FMAU. The high accumulation and the uptake ratio (specificity) of [^18^F]FFAU in tk-positive cells - along with its in vivo stability and favorable biodistribution characteristics, suggested that this probe might be superior to other agents previously studied in the HT-29 cell line.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%29FFAU%20AND%20%28dog%20OR%20sheep%20OR%20pig%20OR%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%29FFAU%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%29FFAU%20AND%20human)]

No publication is currently available.

## References

1 Moolten F.L., Wells J.M., Heyman R.A., Evans R.M. (1990). Lymphoma regression induced by ganciclovir in mice bearing a herpes thymidine kinase transgene. Hum Gene Ther.
2 Oldfield E.H., Ram Z., Culver K.W., Blaese R.M., DeVroom H.L., Anderson W.F. (1993). Gene therapy for the treatment of brain tumors using intra-tumoral transduction with the thymidine kinase gene and intravenous ganciclovir. Hum Gene Ther.
3 Spadari S., Maga G., Focher F., Ciarrocchi G., Manservigi R., Arcamone F., Capobianco M., Carcuro A., Colonna F., Iotti S., et al. (1992). L-thymidine is phosphorylated by herpes simplex virus type 1 thymidine kinase and inhibits viral growth. J Med Chem.
4 Tjuvajev J.G., Avril N., Oku T., Sasajima T., Miyagawa T., Joshi R., Safer M., Beattie B., DiResta G., Daghighian F., Augensen F., Koutcher J., Zweit J., Humm J., Larson S.M., Finn R., Blasberg R. (1998). Imaging herpes virus thymidine kinase gene transfer and expression by positron emission tomography. Cancer Res.
5 Blasberg R.G., Tjuvajev J.G. (1999). Herpes simplex virus thymidine kinase as a marker/reporter gene for PET imaging of gene therapy. Q J Nucl Med.
6 Haberkorn U., Altmann A., Morr I., Knopf K.W., Germann C., Haeckel R., Oberdorfer F., van Kaick G. (1997). Monitoring gene therapy with herpes simplex virus thymidine kinase in hepatoma cells: uptake of specific substrates. J Nucl Med.
7 Alauddin M.M., Conti P.S., Mazza S.M., Hamzeh F.M., Lever J.R. (1996). 9-[(3-[18F]-fluoro-1-hydroxy-2-propoxy)methyl]guanine ([18F]-FHPG): a potential imaging agent of viral infection and gene therapy using PET. Nucl Med Biol.
8 Tjuvajev J.G., Doubrovin M., Akhurst T., Cai S., Balatoni J., Alauddin M.M., Finn R., Bornmann W., Thaler H., Conti P.S., Blasberg R.G. (2002). Comparison of radiolabeled nucleoside probes (FIAU, FHBG, and FHPG) for PET imaging of HSV1-tk gene expression. J Nucl Med.
9 Alauddin M.M., Shahinian A., Park R., Tohme M., Fissekis J.D., Conti P.S. (2004). Synthesis and evaluation of 2'-deoxy-2'-18F-fluoro-5-fluoro-1-beta-D-arabinofuranosyluracil as a potential PET imaging agent for suicide gene expression. J Nucl Med.
10 Coderre J.A., Santi D.V., Matsuda A., Watanabe K.A., Fox J.J. (1983). Mechanism of action of 2',5-difluoro-1-arabinosyluracil. J Med Chem.